# [^177^Lu]-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)

Chemical name: | [^177^Lu]-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)
Abbreviated name: | [^177^Lu]MeO-DOTA-L8A4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, functions, and signal transduction pathways of the various transmembrane epidermal growth factor receptors (EGFRs) are described elsewhere (1-3). The EGFRs are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (2, 3). Overexpression of the EGFR in tumors has been attributed to cellular amplification of the receptor gene, and this phenomenon may result in the production of a mutated receptor in the cell (2, 4). In addition, overexpression of the EGFR in tumors usually indicates a poor clinical prognosis for a cancer patient (4). The most common mutation observed in the receptor is the deletion of an extracellular domain segment of the EGFR, including the ligand-binding region, and this generates a variant known as EGFRvIII or de2-7 EGFR (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy was reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to a ligand due to the absence of a ligand-binding site, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain transformed cells, several anti-EGFR antibodies (http://google2.fda.gov/search?q=anti-EGFR+antibodies+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6) that inhibit the activity of this receptor and small molecule drugs (http://google2.fda.gov/search?q=EGFR+Tyrosine+kinase+inhibitor&spell=1&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&site=FDAgov&access=p) that block the downstream TK signaling pathway were developed and have been approved by the United States Food and Drug Administration for the treatment of certain cancers (2). The antibodies are designed to target the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which leads to downregulation of the EGFR on the cell surface. However, because EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). Hence, a monoclonal antibody (mAb), designated mAb806 and specifically targets the EGFRvIII, was generated and has been characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated ch806, was developed and evaluated in a phase I clinical trial involving patients with cancerous tumors that overexpressed the EGFRvIII. Results from this trial indicated that ch806 can be a suitable biotherapeutic agent to treat cancers (4). Various studies performed with mAb806 or ch806 are described in separate chapters of MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ch806%20AND%20micad%5Bbook%5D).

Studies are also in progress with another anti-EGFRvIII mAb, L8A4, to develop a radioimmunotherapeutic (RIT) agent for the treatment of cancer (9, 10). In a recent study, the use of acyclic ([(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A''-DTPA) and 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) as well as the macrocyclic ligands (S)-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) and α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) was evaluated for the labeling of L8A4 with ^177^Lu, which was considered suitable to generate an RIT agent against cancer (10). The characteristics of the various ^177^Lu-labeled conjugates of L8A4 ([^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4) were compared to the characteristics of L8A4 labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB-L8A4) under in vitro (9) and in vivo (10) conditions.

This chapter describes results obtained from the in vitro and the biodistribution studies performed with [^177^Lu]-MeO-DOTA-L8A4 in athymic mice bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors. Results obtained with [^125^I]SGMIB-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-CHX-A''-DTPA-L8A4 , [^177^Lu]-C-DOTA-L8A4 and are presented in separate chapters of MICAD (www.micad.nih.gov) (11-14).

### Other Sources of Information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Other chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20L8A4%20antibody&cmd=DetailsSearch)]

The preparation, purification, characterization, the conjugation of L8A4 with MeO-DOTA or C-DOTA and the radiolabeling of MeO-DOTA-L8A4 or C-DOTA-L8A4 with ^177^Lu are discussed by Hens et al. (10). The production of [^125^I]SGMIB-L8A4 (labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB)) is also described by Hens et al. (10). The radiochemical yield (RCY) of [^177^Lu]MeO-DOTA-L8A4 and [^177^Lu]C-DOTA-L8A4 was 80% and 73%, respectively (9). The RCY of [^125^I]SGMIB-L8A4 and the purity of the three labeled mAbs was not reported. The specific activity (SA) of [^177^Lu]MeO-DOTA-L8A4 and [^177^Lu]-C-DOTA-L8A4 was reported to be 0.033 MBq/6.6 pmol (0.9 μCi/6.6 pmol) and 0.037 MBq/6.6 pmol (1.0 μCi/6.6 pmol), respectively. The SA of [^125^I]SGMIB-L8A4 varied from 0.111–0.185 MBq/6.6 pmol (3–5 μCi/6.6 pmol) to 0.026–0.118 MBq/6.6 pmol (0.7–3.2 μCi/6.6 pmol). The three labeled mAbs were shown to elute as a single peak with L8A4 and had a similar retention time as the native mAb when analyzed with a size-exclusion column using high performance liquid chromatography. Each molecule of MeO-DOTA-L8A4 and C-DOTA-L8A4 were determined to bear 2.7 and 3.1 moieties of MeO-DOTA and C-DOTA, respectively (9, 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a magnetic bead assay, the immunoreactive fractions of [^177^Lu]-MeO-DOTA-L8A4 and [^177^Lu]-C-DOTA-L8A4 were determined to be 70% and 63%, respectively, compared to between 60% to 71% for [^125^I]SGMIB-L8A4 (9). A cell internalization assay with U87MG.∆EGFR cells showed that internalization of [^177^Lu]-MeO-DOTA-L8A4 and [^177^Lu]-C-DOTA-L8A4 increased from ~5% and ~10%, respectively, at 1 h to ~33% and ~35%, respectively, at 24 h post exposure. In contrast internalization of the ^125^I-labeled mAb peaked to ~10% of the original cell-bound radioactivity at 1 h after exposure and was reduced to ~1% of the original value by 24 h after exposure.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-MeO-DOTA-L8A4, [^177^Lu]-C-DOTA-L8A4, [^177^Lu]-CHX-A''-DTPA-L8A4 and [^177^Lu]-1B4M-DTPA-L8A4 was studied in athymic mice (n = 5 animals/group) bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors and compared it to that of [^125^I]SGMIB-L8A4 as described by Hens et al. (10). The different groups of animals were co-injected (route of injection not reported) with a mixture of the respective ^177^Lu and the ^125^I- labeled mAbs. The rodents were euthanized at 1, 4, and 8 days post injection (p.i.) of the radio-labeled mAbs and all major organs were harvested from the animals. Radioactivity incorporated in the various organs was counted using a dual-channel automated gamma counter and the data was presented as percent of injected dose per gram tissue (% ID/g).

With [^177^Lu]-MeO-DOTA-L8A4 the amount of radioactivity in the blood was 15.35 ± 2.41% ID/g at 1 day p.i. and was reduced to 0.70 ± 0.62% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited accumulation of between 2.75 ± 0.40% ID/g (bone) and 7.88 ± 1.56% ID/g (liver); by 8 days p.i. the amount of label in all these organs decreased to between 0.43 ± 0.27% ID/g (lungs) and 2.89 ± 0.71% ID/g (Liver). The amount of tracer detected in the muscles was 1.65 ± 0.35% Id/g at 1 day p.i. and was reduced to 0.15 ± 0.08% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 38.77 ± 8.55% ID/g at 1 day p.i. and decreased to 10.37 ± 4.05% ID/g by 8 days p.i. The tumor/normal tissue radioactivity uptake ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 5, 6, 5, 80, and 15, respectively, at 1 day p.i. and approximately 4, 6, 4, 350 and 15, respectively at 8 days p.i.

With [^177^Lu]-C-DOTA-L8A4 the amount of radioactivity in the blood was 10.95 ± 1.50% ID/g at 1 day p.i. and was reduced to 1.33 ± 1.60% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited accumulation of between 4.21 ± 1.28% ID/g (lungs) and 13.00 ± 4.79% ID/g (liver); by 8 days p.i. the amount of label in all these organs decreased to between 0.72 ± 0.67% ID/g (lungs) and 5.39 ± 2.54% ID/g (Liver). The amount of tracer detected in the muscles was 1.32 ± 0.26% Id/g at 1 day p.i. and was reduced to 0.25 ± 0.16% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 23.52 ± 3.14% ID/g at 1 day p.i. and decreased to 7.47 ± 6.89% ID/g by 8 days p.i. The tumor/normal tissue radioactivity uptake ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 2, 5.5, 2, 80, and 5, respectively, at 1 day p.i. and approximately 1.2, 5, 1.2, 120 and 2, respectively at 8 days p.i.

With [^177^Lu]-1B4M-DTPA-L8A4 the amount of radioactivity in the blood was 19.78 ± 2.94% ID/g at 1 day p.i. and this was reduced to 1.35 ± 0.94% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited an accumulation of between 8.36 ± 0.74% ID/g (liver) and 3.58 ± 1.44% ID/g (bone) and the by 8 days p.i. amount of label in all these organs, except the bone, decreased to between 0.93 ± 0.45% ID/g (lungs) and 4.16 ± 0.54% ID/g (Liver) (10). During this period the incorporation of radioactivity in the bone decreased from 3.58 ± 1.44% ID/g at 1 day p.i. to 1.82 ± 0.52% ID/g at 8 days p.i. The amount of tracer accumulated in the muscles was 1.64 ± 0.08% Id/g at 1 day p.i. and was reduced to 0.30 ± 0.07% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 31.58 ± 6.60% ID/g at 1 day p.i. and decreased to 15.27 ± 5.16% ID/g by 8 days p.i. The tumor/normal tissue radioactivity uptake ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 3.8, 4, 4, 55, and 10, respectively, at 1 day p.i. and approximately 3.8, 6, 4, 200 and 8, respectively at 8 days p.i.

With [^177^Lu]-CHX-A''-DTPA-L8A4 the amount of radioactivity in the blood was 15.18 ± 3.30% ID/g at 1 day p.i. and this was was reduced to 0.99 ± 0.71% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited accumulation of between 8.53 ± 1.86% ID/g (liver) and 5.98 ± 1.86% ID/g (spleen) and the by 8 days p.i. amount of label in all these organs, except the bone, decreased to between 0.56 ± 0.23% ID/g (lungs) and 4.45 ± 0.87% ID/g (Liver). During this period the incorporation of radioactivity in the bone increased from 5.95 ± 1.27% ID/g at 1 day p.i. to 7.56 ± 1.88% ID/g at 8 days p.i. This phenomenon was attributed to the bone seeking character of ^177^Lu indicating that [^177^Lu]-CHX-A''-DTPA-L8A4 may not be suitable detection agent for EGFRvIII expressing tumors. The amount of tracer accumulated in the muscles was 1.30 ± 0.44% Id/g at 1 day p.i. and was reduced to 0.19 ± 0.05% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 36.28 ± 6.60% ID/g at 1 day p.i. and decreased to 8.67 ± 3.42% ID/g by 8 days p.i. The tumor/normal tissue radioactivity uptake ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 4, 6, 4, 95, and 6, respectively, at 1 day p.i. and approximately 2, 5, 2, 200 and 2, respectively at 8 days p.i.

With [^125^I]SGMIB-L8A4 the amount of radioactivity in the blood at 1 day p.i. was 18.78 ± 2.24% ID/g and decreased to 1.29 ± 0.87% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, and lungs exhibited accumulation between 5% and 7% ID/g and the amount of label in all these organs decreased to ~0.5% ID/g by 8 days p.i. The amount of tracer detected in the muscles and bones was ~1.5 and ~3.5% ID/g, respectively, at 1 day p.i.; by 8 days p.i., accumulation decreased to ~0.15% ID/g and ~0.33% ID/g, respectively, in these tissues. The tumor had a radioactivity accumulation of 21.64 ± 4.53% ID/g at 1 day p.i., which decreased to 2.86 ± 0.98% ID/g by 8 days p.i. The tumor/normal tissue radioactivity uptake ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 6, 8, 6, 60, and 10, respectively, at 1 day p.i. and approximately 7, 8, 7, 60 and 6, respectively, at 8 days p.i.

Table 1: Summary of tumor/normal tissue radioactivity uptake ratios for various organs obtained with the [ ^ 125 ^ I]SGMIB-L8A4, [ ^ 177 ^ Lu]MeO-DOTA-L8A4, [ ^ 177 ^ Lu]C-DOTA-L8A4, [ ^ 177 ^ Lu]1B4M-DTPA-L8A4 and [ ^ 177 ^ Lu]CHX-A”-DTPA-L8A4. Data obtained from Figure 5 in Hens et al. ( 10 ).

Conjugated mAb | Liver | | Kidney | | Spleen | | Brain | | Bone
Conjugated mAb | Time after labeled mAb injection
Conjugated mAb | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days
Conjugated mAb | Tumor-to-normal tissue ratio
[ ^ 125 ^ I]SGMIB-L8A4 | 6 | 7 | 8 | 8 | 6 | 7 | 60 | 60 | 10 | 6
[ ^ 177 ^ Lu]MeO-DOTA-L8A4 | 5 | 4 | 6 | 6 | 5 | 4 | 80 | 350 | 15 | 15
[ ^ 177 ^ Lu]C-DOTA-L8A4 | 2 | 1.2 | 5.5 | 5 | 2 | 1.2 | 80 | 120 | 5 | 2
[ ^ 177 ^ Lu]1B4M-DTPA-L8A4 | 3.8 | 3.8 | 4 | 6 | 4 | 4 | 55 | 200 | 10 | 8
[ ^ 177 ^ Lu]CHX-A”-DTPA-L8A4 | 4 | 2 | 6 | 5 | 4 | 2 | 95 | 200 | 6 | 2

Based on the results presented in Table 1, [^177^Lu]MeO-DOTA-L8A4 and [^177^Lu]1B4M-DTPA-L8A4 appear to be superior compared to the other mAbs, including [^125^I]SGMIB-L8A4, for the detection of EGFRvIII overexpressing tumors in rodents because both the mAbs show a lower incorporation of radioactivity in the bones and maintain the tumor-to-normal tissue ratios even at 8 days p.i (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants NS20023 and CA42324.

## References

1 Hasselbalch B., Lassen U., Poulsen H.S., Stockhausen M.T. (2010). Cetuximab insufficiently inhibits glioma cell growth due to persistent EGFR downstream signaling. Cancer Invest.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Hens M., Vaidyanathan G., Welsh P., Zalutsky M.R. (2009). Labeling internalizing anti-epidermal growth factor receptor variant III monoclonal antibody with (177)Lu: in vitro comparison of acyclic and macrocyclic ligands. Nucl Med Biol.
10 Hens M., Vaidyanathan G., Zhao X.G., Bigner D.D., Zalutsky M.R. (2010). Anti-EGFRvIII monoclonal antibody armed with 177Lu: in vivo comparison of macrocyclic and acyclic ligands. Nucl Med Biol.
11 Chopra, A., [125I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 177Lu-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA)) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [177Lu]-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Chopra, A., 177Lu-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.